# [^64^Cu]-1,4,7,10-Tetra-azacyclododecane-N,N’,N’’,N’’’-tetraacetic acid conjugated knottin 2.5F

Chemical name: | [^64^Cu]-1,4,7,10-Tetra-azacyclododecane-N,N’,N’’,N’’’-tetraacetic acid conjugated knottin 2.5F
Abbreviated name: | [^64^Cu]Knottin 2.5F; ^64^Cu-DOTA-2.5F
Synonym:
Agent Category: | Ligand
Target: | α_v_β_3_, α_v_β_5_, and α_5_β_1_ integrin receptors
Target Category: | Receptors
Method of detection: | Positron emission tomography (PET)
Source of signal / contrast: | ^64^Cu
Activation: | No
Studies: | - In vitro; - Rodents | Structure not available in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=knottin+peptides)]

Integrin receptors that mediate tumor angiogenesis, growth, and metastasis through a complex network of signaling pathways are known to be expressed on the surface of cancerous tumor cells and neovasculature (1-3). Because of their role in tumor development and progression, inhibition of integrin receptor activity is being actively investigated in clinical trials for the treatment (http://clinicaltrials.gov/ct2/results?term=integrin+inhibitors) and imaging (http://clinicaltrials.gov/ct2/results?term=integrin+imaging) of various cancers (4, 5). Non-invasive imaging probes can be used to determine not only the efficacy of integrin-targeted anti-cancer drugs, but also to monitor disease progression and metastasis (6, 7). Although integrin receptors usually bind through the arginine-glycine-aspartic acid (RGD) motif of the extracellular matrix protein ligands, it is the amino acid residues surrounding the RGD motif that determine the receptor specificity and affinity for the ligand (4, 8, 9). As a result of the small size of the drugs, mainly peptides, that target the integrin receptor, it has been challenging to generate peptides containing the RGD motif that have an improved pharmacokinetic behavior, receptor affinity, and tumor uptake for in vivo imaging purposes. Any modification of the peptide structure has yielded integrin-targeted imaging agents that have only a limited advancement and application in the clinics (10, 11). Only one imaging compound with an RGD motif, a radioactive fluorine-labeled cyclic pentapeptide ([^18^F]-galacto-RGD), was determined to be suitable to identify integrin-positive tumors and to investigate α_v_β_3_ integrin expression in humans. However, [^18^F]-galacto-RGD has been shown to have a low tumor uptake, and it generated a high background signal due to accumulation in the liver (12, 13).

In an effort to develop imaging agents for the detection of integrin receptors expressed on tumor cell surface and neovasculature, Kimura et al. (14) used the directed evolution technique (15, 16) to place the integrin-binding RGD motif into a cystine knot peptide (also known as knottin) trypsin inhibitor of the squash plant (Ecballium elaterium) (17). The peptide was reported to have a high affinity for the α_v_β_3_ and α_v_β_5_ or the α_v_β_3_, α_v_β_5_, and α_5_β_1_ integrin receptors. In general, knottins have a core structure containing a disulfide bond, are resistant to proteolysis, have a high thermodynamic stability, and are nonimmunogenic (14). The knottin peptide containing an RGD motif (designated as knottin 2.5F) was labeled with radioactive copper (^64^Cu) to obtain [^64^Cu]knottin 2.5F (^64^Cu-1,4,7,10-tetra-azacyclododecane-N,N’,N’’,N’’’-tetraacetic acid-2.5F (^64^Cu-DOTA-2.5F)) and used to image xenograft tumors in mice with positron emission tomography (PET). It is pertinent to mention here that the amino acid sequence and structure of knottins 2.5D and 2.5F (also studied by Kimura et. al. (14)) are discussed elsewhere (14).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=64Cu+knottin+2%2E5D+synthesis)]

The synthesis of knottin 2.5F was performed with the use of the 9-fluorenylmethylcarbonyl-based solid-phase technique as described by Kimura et al. (14). In addition, two other knottin peptides, FN-RGD2 (for use as positive a control) and FN-RDG2 (negative control) were synthesized using the same technique mentioned above. A third peptide, c(RGDyK), was obtained from commercial sources for use as a second control. The amino acid sequence, structure and properties of the various integrin-binding peptides used for studies described in this chapter are discussed by Kimura et al. (14).

To radiolabel knottin 2.5F, the peptide was mixed with molar excess of an in situ preparation of a sulfosuccinimide ester of DOTA for 1 h at room temperature and then overnight at 4°C (14). By this reaction the chelating agent was attached at the amino terminal of the folded knottin peptide for chelation of the radionuclide (^64^Cu). The final product, a knottin 2.5F-DOTA conjugate, was purified with reverse-phase high-performance liquid chromatography (RP-HPLC) on a C_18_ column as described by Kimura et al. (14). After folding the conjugated peptide as detailed by Kimura et al. (14), the agent was purified with semi-preparative RP-HPLC and freeze-dried for storage at room temperature until required. The peptide purity and molecular mass were confirmed with analytical RP-HPLC and electrospray ionization mass spectrometery. To label with ^64^Cu, the knottin 2.5F-DOTA conjugate was incubated with ^64^CuCl_2_ in 0.1 N sodium acetate buffer (pH 6.3) for 1 h at 45°C. The reaction was terminated by the addition of ethylenediamine tetraacetic acid, and the radiolabeled product was purified with radio-HPLC on a PD-10 column. The purified product was dried, reconstituted in phosphate-buffered saline, and sterilized by filtration. For use as controls, ^64^Cu-labeled FN-RGD2, FN-RDG2, and c(RGDyK) were also respectively synthesized using the protocol described above. The radiochemical yield of the purified products was usually >80% (at least seven reactions/purifications were performed respectively on different days), and the purity was >95% as determined with HPLC. The specific activity of the various ^64^Cu-labeled peptides was not reported.

The stability of ^64^Cu-DOTA-2.5F was determined by exposing it to mouse serum for 1, 4, and 24 h at 37°C (14). Minimal degradation of the radiolabeled peptide was reported at all the time points as determined with HPLC.

Echistatin labeled with radioactive iodine (^125^I-echistatin), used a s a control in some studies, was obtained from a commercial source (14).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=64Cu+knottin+2%2E5D+in+vitro+studies)]

To determine the relative integrin-binding affinities (reported as 50% inhibitory concentration (IC_50_)) of the modified and unmodified peptides, including knottin 2.5F, a competition binding assay was performed with ^125^I-echistatin (a strong antagonist of α_v_β_3_, α_v_β_5_, α_5_β_1_ and α_iib_β_3_ integrins (14)) using U-87MG cells (a human glioblastoma cell line that expresses several types of integrins on the cell surface) as described by Kimura et al. (14). The IC_50_ for DOTA-knottin 2.5F was determined to be 26 ± 5 nmol/L compared with an IC_50_ values of 590 ± 210 nmol/L and 380 ± 190 nmol/L for the control DOTA-conjugated FN-RGD2 and c(RGDyK) peptides, respectively. The negative control peptide, DOTA-FN-RDG2, did not compete with ^125^I-echistatin for binding to the U-87MG cells. The DOTA-conjugated peptides (modified) were reported to have IC_50_ values comparable to the unmodified (not conjugated to DOTA) peptides (14).

The integrin-binding specificity of the DOTA-conjugated knottin peptides was investigated with a competition assay using ^125^I-echistatin (14). Different concentrations (5 and 50 nmol/L) of the unlabeled DOTA-conjugated knottin peptides were respectively incubated with ^125^I-echistatin in microtiter plates coated with detergent-solubalized α_v_β_3_, α_v_β_5_, α_5_β_1_, and α_iib_β_3_ integrin receptors for 3 h at room temperature. The plates were washed three times to remove unbound radioactivity, and the contents were solubalized in 2 N sodium hydroxide to determine the amount of receptor-bound radioactivity. Compared with the FN-RGD2 and c(RGDyK) peptides, the knottin 2.5F peptide exhibited a higher binding (for details see Figure 2A in reference 14) to the different integrin receptors except α_iib_β_3_, which is expressed mainly on the platelet cells (14).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=64Cu+knottin+2%2E5D+rodentia)]

The use of ^64^Cu-DOTA-2.5F as a PET imaging probe was investigated in mice bearing human U-87MG cell xenograft tumors (14). The animals (n = 3 or more for each probe) were injected with the respective ^64^Cu-DOTA-conjugated peptides through the tail vein and imaged 1 h later for up to 24 h. Calibration of the PET images for quantitation purposes was done as described by Wu et. al (18). At 1 h after administration of the labeled peptides, the tumor uptake of ^64^Cu-DOTA-2.5F was higher (4.56 ± 0.64% injected dose/gram tissue (% ID/g)) compared with the control ^64^Cu-DOTA-FN-RGD2 (1.48 ± 0.53% ID/g) and ^64^Cu-DOTA-c(RGDyK) (2.32 ± 0.55% ID/g) peptides. Also, compared with ^64^Cu-DOTA-FN-RGD2 (4.19 ± 0.78% ID/g and 3.59 ± 0.87% ID/g at 1 and 4 h after injection, respectively), a lower uptake of ^64^Cu-DOTA-2.5F (~2% ID/g) was observed in the liver. For the negative control peptide, ^64^Cu-DOTA-FN-RDG2, the tumor accumulation of radioactivity was reported to be 1.09 ± 0.48% ID/g and 0.76 ± 0.33% ID/g at 1 and 4 h after injection, respectively. No competition studies were reported.

For the in vivo biodistribution studies, animals bearing U-87MG cell xenograft tumors (at least three mice per time point) were injected with ^64^Cu-knottin 2.5F through the tail vein, and the amount or radioactivity accumulated in the major organs was determined after 0.5 and 4 h (14). At 0.5 h, varying amounts of radioactivity (<0.5–8.0% ID/g) was detected primarily in the tumor, blood, liver, lungs, kidneys, spleen, intestines, skin, and the stomach (for details see Figure 4C in reference 14). By 4 h after administration, the radioactivity was reduced to between <1% ID/g (liver, lung, spleen, intestines, skin, and stomach) and ~2% ID/g (liver and intestines) and ~4% ID/g (kidneys).

From these studies the investigators concluded that the direct evolution–engineered integrin-binding peptides had a good potential for the detection and diagnosis of various cancers (14).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22%20SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=64Cu+knottin+2%2E5D+Non+Human+Primates)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=64Cu+knottin+2%2E5D+Human+Studies)]

No references are currently available.

## Supplemental Information

[Disclaimers]

## NIH Support

Some of the work presented in this chapter was supported by National Cancer Institute grants 5K01 CA104706, 5R25T CA118681, and R25T CA118681 and a National Institutes of Health grant P50 CA114747.

## References

1 Legate K.R., Wickstrom S.A., Fassler R. (2009). Genetic and cell biological analysis of integrin outside-in signaling. Genes Dev.
2 Pontier S.M., Muller W.J. (2009). Integrins in mammary-stem-cell biology and breast-cancer progression--a role in cancer stem cells?. J Cell Sci.
3 Streuli C.H. (2009). Integrins and cell-fate determination. J Cell Sci.
4 Moschos S.J., Drogowski L.M., Reppert S.L., Kirkwood J.M. (2007). Integrins and cancer. Oncology.
5 Fujita Y., Abe R., Shimizu H. (2008). Clinical approaches toward tumor angiogenesis: past, present and future. Curr Pharm Des.
6 Zaccaro L., Del Gatto A., Pedone C., Saviano M. (2009). Peptides for tumour therapy and diagnosis: current status and future directions. Curr Med Chem.
7 Haubner R., Decristoforo C. (2009). Radiolabelled RGD peptides and peptidomimetics for tumour targeting. Front Biosci.
8 Chen, C.Y., J.H. Shiu, Y.H. Hsieh, Y.C. Liu, Y.C. Chen, Y.C. Chen, W.Y. Jeng, M.J. Tang, S.J. Lo, and W.J. Chuang, Effect of D to E mutation of the RGD motif in rhodostomin on its activity, structure, and dynamics: Importance of the interactions between the D residue and integrin. Proteins, 2009
9 Manzoni, L., L. Belvisi, D. Arosio, M. Civera, M. Pilkington-Miksa, D. Potenza, A. Caprini, E.M. Araldi, E. Monferini, M. Mancino, F. Podesta, and C. Scolastico, Cyclic RGD-Containing Functionalized Azabicycloalkane Peptides as Potent Integrin Antagonists for Tumor Targeting. ChemMedChem, 2009
10 Cai W., Rao J., Gambhir S.S., Chen X. (2006). How molecular imaging is speeding up antiangiogenic drug development. Mol Cancer Ther.
11 Haubner R. (2006). Alphavbeta3-integrin imaging: a new approach to characterise angiogenesis?. Eur J Nucl Med Mol Imaging.
12 Haubner R., Weber W.A., Beer A.J., Vabuliene E., Reim D., Sarbia M., Becker K.F., Goebel M., Hein R., Wester H.J., Kessler H., Schwaiger M. (2005). Noninvasive visualization of the activated alphavbeta3 integrin in cancer patients by positron emission tomography and [18F]Galacto-RGD. PLoS Med.
13 Beer A.J., Haubner R., Sarbia M., Goebel M., Luderschmidt S., Grosu A.L., Schnell O., Niemeyer M., Kessler H., Wester H.J., Weber W.A., Schwaiger M. (2006). Positron emission tomography using [18F]Galacto-RGD identifies the level of integrin alpha(v)beta3 expression in man. Clin Cancer Res.
14 Kimura R.H., Cheng Z., Gambhir S.S., Cochran J.R. (2009). Engineered knottin peptides: a new class of agents for imaging integrin expression in living subjects. Cancer Res.
15 Otten L.G., Quax W.J. (2005). Directed evolution: selecting today's biocatalysts. Biomol Eng.
16 Leemhuis H., Kelly R.M., Dijkhuizen L. (2009). Directed evolution of enzymes: Library screening strategies. IUBMB Life.
17 Favel A., Mattras H., Coletti-Previero M.A., Zwilling R., Robinson E.A., Castro B. (1989). Protease inhibitors from Ecballium elaterium seeds. Int J Pept Protein Res.
18 Wu Y., Zhang X., Xiong Z., Cheng Z., Fisher D.R., Liu S., Gambhir S.S., Chen X. (2005). microPET imaging of glioma integrin {alpha}v{beta}3 expression using (64)Cu-labeled tetrameric RGD peptide. J Nucl Med.